# D-Cys-D-Asp-Gly-HCit-Gly-Pro-Gln-D-Cys-Ebes-Ebes-Lys-Cy5.5

Chemical name: | D-Cys-D-Asp-Gly-HCit-Gly-Pro-Gln-D-Cys-Ebes-Ebes-Lys-Cy5.5
Abbreviated name: | OA02-Cy5.5
Synonym:
Agent Category: | Peptide
Target: | Integrin α_3_β_1_
Target Category: | Receptor binding
Method of detection: | Optical, Near-Infrared
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=152013007), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=152013006) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3675) for more information about integrin α_3_β_1_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02)]

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background interference as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity as a result of low infrared background interference, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging.

Integrins are a family of cell-surface heterodimeric glycoproteins that mediate diverse biological events involving cell–cell and cell–matrix interactions (3). They consist of an α and a β subunit. They are important for cell adhesion and signal transduction. The α_3_β_1_ integrin plays an important role in normal lung, kidney, cerebral cortical, and epithelial development (4). On the other hand, it affects tumor growth, tumor invasiveness, and metastasis as the α_3_β_1_ integrin is strongly expressed on tumor cells (5, 6). D-Cys-D-Asp-Gly-HCit-Gly-Pro-Gln-D-Cys (OA02) was identified to bind to the α_3_ integrin on human ovarian cancer cells using one-bead-one-compound combinatorial libraries (7, 8). OA02 was conjugated with Cy5.5 to study in vivo biodistribution of the tracer in tumor-bearing mice (9). Cy5.5 is a NIR fluorescent dye with an absorbance maximum at 675 nm and emission maximum at 694 nm with a high extinction coefficient of 250,000 (mol/L)^-1^cm^-1^. OA02-Cy5.5 was found to have a high specific accumulation in α_3_β_1_-positve ES-2 human ovarian tumor cells in nude mice.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02+and+synthesis)]

Cy5.5 monofunctional N-hydroxysuccinimide (NHS) ester was used to conjugate D-Cys-D-Asp-Gly-HCit-Gly-Pro-Gln-D-Cys-Ebes-Ebes-Lys using solid-phase synthesis to form OA02-Cy5.5 (9). The NHS ester of Cy5.5 reacted with the ε-amino group of the lysine. The peak containing the OA02-Cy5.5 conjugate was analyzed by matrix-assisted laser desorption/ionization-time-of-flight mass spectrometry. The measured mass was m/z 2,457.2, which was ~1 Cy5.5/OA02. The chemical purity was >90%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02+and+in+vitro)]

Receptor-mediated endocytosis of OA02-biotin in SKOV-3 human ovarian tumor cells (α_3_-positive) was observed by fluorescent microscopy (9). The staining was confined to the cell membrane and cytoplasm. On the other hand, Raji B-cell lymphomas (α_3_-negative) did not show any staining.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02+and+rodentia)]

Biodistribution studies of OA02-Cy5.5 were evaluated in nude mice bearing an ES-2 subcutaneous xenograft in the left flank and a Raji subcutaneous xenograft in the right flank. Images were obtained after injection of 20 µg (8.14 nmol) OA02-Cy5.5 (9). The background fluorescent intensity was 225 ± 15 arbitrary units (AU) for both tumors. The ES-2 tumor uptake of OA02-Cy5.5 was 6,032 ± 4,640 AU at 15 min and 5,526 ± 3,696 AU at 70 min, whereas the Raji tumor uptake was 2,685 ± 1,103 AU at 15 min and 2,786 ± 1,583 AU at 70 min. There was a gradual clearance of the signal from the system via the kidneys. The fluorescent intensity decreased to ~2,000 AU at 1,440 min for both tumors. The tracer uptake in both tumors could be reduced to background level (~700 AU) at 70 min by pre-administration of anti-α_3_ monoclonal antibody 30 min before OA02-Cy5.5 injection. Ex vivo imaging showed that most of the fluorescent signal intensity was from the ES-2 tumor, urinary bladder, and kidneys.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=OA02+and+human)]

No publication is currently available.

## NIH Support

R33 CA89706, 5-T32-RR07038

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Schellenberger E.A., Ripoll J., Yessayan D., Graves E., Bogdanov A., Josephson L., Weissleder R. (2004). Visualization of antitumor treatment by means of fluorescence molecular tomography with an annexin V-Cy5.5 conjugate. Proc Natl Acad Sci U S A.
3 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
4 Hynes R.O. (2002). Integrins: bidirectional, allosteric signaling machines. Cell.
5 Albelda S.M., Mette S.A., Elder D.E., Stewart R., Damjanovich L., Herlyn M., Buck C.A. (1990). Integrin distribution in malignant melanoma: association of the beta 3 subunit with tumor progression. Cancer Res.
6 Hynes R.O. (2002). A reevaluation of integrins as regulators of angiogenesis. Nat Med.
7 Aina O.H., Liu R., Sutcliffe J.L., Marik J., Pan C.X., Lam K.S. (2007). and From Combinatorial Chemistry to Cancer-Targeting Peptides. Mol Pharm.
8 Aina O.H., Marik J., Liu R., Lau D.H., Lam K.S. (2005). Identification of novel targeting peptides for human ovarian cancer cells using "one-bead one-compound" combinatorial libraries. Mol Cancer Ther.
9 Aina O.H., Marik J., Gandour-Edwards R., Lam K.S. (2005). Near-infrared optical imaging of ovarian cancer xenografts with novel alpha 3-integrin binding peptide "OA02". Mol Imaging.